# ^99m^TcO-N,N-Dimethylglycyl-L-lysinyl-L-cysteinylamide-8-amino-3,6-dioxaoctanoic-probestin

Chemical name: | ^99m^TcO-N,N-Dimethylglycyl-L-lysinyl-L-cysteinylamide-8-amino-3,6-dioxaoctanoic-probestin
Abbreviated name: | ^99m^TcO-N_3_S-PEG_2_-probestin
Synonym:
Agent category: | Peptide
Target: | Aminopeptidase N (APN, also known as CD13)
Target category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (4). This process is driven by the tumor's overproduction of angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (5-7). Aminopeptidase N (APN, CD13) is a membrane-bound glycoprotein with MMP activity that cleaves unsubstituted N-terminal amino acids with neutral side chains from peptides (8). APN has been shown to play a role in tumor angiogenesis, invasion, and metastasis (9). In addition to endothelial cells of angiogenic vessels, most cells of myeloid origin, epithelial cells, fibroblasts, and smooth muscle cells also express CD13 (10, 11). High levels of CD13 expression were found in solid tumors and tumor vasculatures. Probestin ((2S,3R)-3-amino-2-hydroxy-4-phenylbutanoyl-L-Leu-L-Pro-L-Pro) is a competitive inhibitor of APN with an inhibition constant (K_i_) value of 20 nM. Pathuri et al. (12) prepared ^99m^TcO-N,N-dimethylglycyl-L-lysinyl-L-cysteinylamide-8-amino-3,6-dioxaoctanoic-probestin (^99m^TcO-N_3_S-PEG_2_-probestin) as a single-photon emission computed tomography (SPECT) for imaging APN expression in tumors in mice.

### Related Resource Links:

- Chapters in MICAD (APN (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Aminopeptidase%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (APN (http://www.ncbi.nlm.nih.gov/gene/290))
- Articles in Online Mendelian Inheritance in Man (OMIM) (APN (http://omim.org/entry/151530))
- Clinical trials (APN (http://www.clinicaltrials.gov/ct2/results?term=cd13))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin+synthesis)]

N_3_S-PEG_2_-Probestin was prepared with solid-phase peptide synthesis (12). ^99m^Tc as pertechnetate (370 MBq (10 mCi)) was added to a solution of N_3_S-PEG_2_-probestin (100 µg) containing sodium gluconate and SnCl_2_. The mixture was incubated for 30 min at 25°C. The labeling efficiency of ^99m^Tc incorporation was 50%–60% with >98% radiochemical purity after high-performance liquid chromatography. The specific activity of ^99m^TcO-N_3_S-PEG_2_-probestin was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin+in+vitro)]

Histoimmunostaining of CD13 was performed on HT-1080 and MCF-7 cancer cell lines (13). The APN enzyme was detected on the cell surface of HT-1080 tumor cells, whereas expression in MCF-7 tumor cells was only at the level of background staining. The APN activity in HT-1080 cells could be blocked with anti-CD13 antibodies.

Pathuri et al. (12) performed in vitro APN inhibition cell assays with HT-1080 cells and Ala-p-nitroanilide as the APN substrate for 30 min at 25°C. The 50% inhibition values were 797, 39.6, and 23.6 µM for probestin, ReO-PEG_2_-probestin, and ReO-N_3_S-PEG_2_-probestin, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin+rodentia)]

Pathuri et al. (12) performed ex vivo biodistribution studies of 1.28 MBq (35 μCi) ^99m^TcO-N_3_S-PEG_2_-probestin at 1 h after injection in nude mice (n = 4) bearing HT-1080 fibrosarcoma tumors. The tumor accumulation of radioactivity was 2.88 ± 0.64% injected dose per gram (ID/g). The tumor/blood and tumor/muscle ratios were 4.8 and 5.3, respectively. The radioactivity levels in the kidney (48% ID/g), liver (12% ID/g), and intestine (5% ID/g) were higher than the radioactivity in the spleen (2.4% ID/g), stomach (1.3% ID/g), heart (1.2% ID/g), and lung (0.9% ID/g). No target specificity studies were performed.

SPECT imaging analysis was performed in nude mice bearing the HT-1080 tumors after injection of 25.2 MBq (0.68 mCi) ^99m^TcO-N_3_S-PEG_2_-probestin (12). The tumor was clearly visualized at 0.5 h, along with the kidneys and urinary bladder. At 3 h, the tumor and intestine were still visualized along with a lower radioactivity in the kidneys and urinary bladder. Planar images showed radioactivity in the tumor, thymus, kidneys, liver, and intestine at 1 h after tracer injection. Co-injection of excess ReO-N_3_S-PEG_2_-probestin blocked radioactivity in the tumor, thymus, and kidneys, whereas there was an increase in radioactivity in the liver and intestine.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Probestin+human)]

No publication is currently available.

## NIH Support

S10 RR025652

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
5 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
6 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
7 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
8 Riemann D., Kehlen A., Langner J. (1999). CD13--not just a marker in leukemia typing. Immunol Today.
9 Sato Y. (2004). Role of aminopeptidase in angiogenesis. Biol Pharm Bull.
10 Corti A., Curnis F., Arap W., Pasqualini R. (2008). The neovasculature homing motif NGR: more than meets the eye. Blood.
11 Curnis F., Arrigoni G., Sacchi A., Fischetti L., Arap W., Pasqualini R., Corti A. (2002). Differential binding of drugs containing the NGR motif to CD13 isoforms in tumor vessels, epithelia, and myeloid cells. Cancer Res.
12 Pathuri G., Hedrick A.F., Disch B.C., Doan J.T., Ihnat M.A., Awasthi V., Gali H. (2012). Synthesis and Evaluation of Novel Tc-99m Labeled Probestin Conjugates for Imaging APN/CD13 Expression In Vivo. Bioconjug Chem.
13 von Wallbrunn A., Waldeck J., Holtke C., Zuhlsdorf M., Mesters R., Heindel W., Schafers M., Bremer C. (2008). In vivo optical imaging of CD13/APN-expression in tumor xenografts. J Biomed Opt.